# ^111^In-Labeled (7S)-26-(4-((1-((1-carboxy-5-(2-(4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecan-1-yl)acetamido)pentyl)amino)-1-oxo-6-(1-((7S)-1,3,7,22-tetracarboxy-5,13,20-trioxo-4,6,12,21-tetraazahexacosan-26-yl)-1H-1,2,3-triazole-4-carboxamido)hexan-2-yl)carbamoyl)-1H-1,2,3-triazol-5-yl)-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid

Chemical name: | ^111^In-Labeled (7S)-26-(4-((1-((1-carboxy-5-(2-(4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecan-1-yl)acetamido)pentyl)amino)-1-oxo-6-(1-((7S)-1,3,7,22-tetracarboxy-5,13,20-trioxo-4,6,12,21-tetraazahexacosan-26-yl)-1H-1,2,3-triazole-4-carboxamido)hexan-2-yl)carbamoyl)-1H-1,2,3-triazol-5-yl)-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid | [image]
Abbreviated name: | [^111^In]3 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Prostate-specific membrane antigen (PSMA) | [image]
Target Category: | Antigens | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^111^In]3 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=PSMA+and%20molecular%20imaging)]

^111^In-Labeled (7S)-26-(4-((1-((1-carboxy-5-(2-(4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecan-1-yl)acetamido)pentyl)amino)-1-oxo-6-(1-((7S)-1,3,7,22-tetracarboxy-5,13,20-trioxo-4,6,12,21-tetraazahexacosan-26-yl)-1H-1,2,3-triazole-4-carboxamido)hexan-2-yl)carbamoyl)-1H-1,2,3-triazol-5-yl)-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid, abbreviated as [^111^In]3, was synthesized by Banerjee et al. for use in single-photon emission computed tomography (SPECT) of tumors expressing prostate-specific membrane antigen (PSMA) (1).

PSMA is a type II transmembrane glycoprotein with three structural domains, including a 19-amino-acid intracellular domain, a 24-amino-acid transmembrane domain, and a large 707-amino-acid extracellular domain (2, 3). Two site-specific carboxypeptidase activities have been assigned to PSMA: N-acetylated α-linked acidic dipeptidase, which hydrolyzes the neuropeptide N-acetyl-aspartyl-glutamate (NAAG) in the brain to regulate release of neurotransmitters, and folate hydrolase activity, which is characterized by the cleavage of terminal glutamates from poly- and gamma-glutamated folates, which play a role in the cellular uptake of dietary folate (2). PSMA has been found to be expressed in the prostate at a level 1,000-fold greater than that in other tissues, and many folds higher in prostate cancer than in normal and benign prostate tissues (4, 5). High-grade and hormone-insensitive tumors have the greatest PSMA expression. PSMA is also consistently and abundantly expressed on the neovascular endothelium in a wide variety of human solid tumors, but not in blood vessels in normal tissues. These features of PSMA make it an optimal target for developing imaging and therapy strategies for prostate cancer (6).

Besides antibodies and antibody fragments, low molecular weight compounds have also been intensively tested as PSMA inhibitors and as PSMA-targeted imaging agents (6, 7). These compounds can be largely classified into two types: ureas and phosphoramidates (7). Both types of compounds possess a terminal glutamate at the P1' position, which enables productive binding with PSMA. They are also amenable to modification with bulky substituents that interact with the arginine patch or tunnel region on PSMA. Investigators have synthesized a series of ureas, including [^18^F]DCFBC, [^18^F]DCFPyL, and [^111^In]3 (1, 7, 8). [^111^In]3 is a bivalent compound that was synthesized by incorporating a PSMA-binding Lys-Glu urea motif for exploiting click chemistry and a second lysine residue for subsequent modification with an imaging or therapeutic moiety (1). Studies have shown that these radiolabeled PSMA inhibitors have desirable properties as imaging agents for prostate cancer imaging in animal models (1, 7, 8). This chapter summarizes the data obtained with [^111^In]3. In another chapter, the data obtained with [^18^F]DCFPyL are summarized. The data obtained with [^18^F]DCFBC can be reviewed in the chapter on [^18^F]DCFBC (http://www.ncbi.nlm.nih.gov/books/NBK23394/) in MICAD.

### Related Resource Links:

- PSMA-targeted imaging agents (http://www.ncbi.nlm.nih.gov/books/?term=PSMA+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/gene/2346))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/omim/600934))
- PSMA-related clinical trials (http://www.clinicaltrials.gov/ct2/results?term=PSMA&Search=Search) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22207391)]

Banerjee et al. described the synthesis of precursor compounds in detail, including monovalent compound 1 ((3S,7S)-26-azido-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid), bivalent compound 2 ((7S)-26-(4-((1-((5-amino-1-carboxypenty l)amino)-1-oxo-6-(1-((7S)-1,3,7,22-tetracarboxy-5,13,20-trioxo-4,6,12,21-tetraazahexacosan-26-yl)-1H-1,2,3-triazole-4-carboxamido)hexan-2-yl)carbamoyl)-1H-1,2,3-triazol-5-yl)-5,13,20-trioxo-4,6,12,21-tetraazahexacosane-1,3,7,22-tetracarboxylic acid), and DOTA-chelated bivalent urea compound 3 (1). Compound 3 (50–70 µg) was labeled with ^111^In (111–148 MBq, 3–4 mCi) via incubation for 20 h at 95°C in 0.3 M NaOAc buffer. The radiochemical yield of [^111^In]3 was 70%–90% yield, and its specific radioactivity was 8.4–204.4 GBq/μmol (0.23–5.52 mCi/µmol). The radiochemical purity was >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22207391)]

The PSMA enzyme inhibition potency of compounds 1–3 was determined with a modified Amplex Red glutamic acid assay after incubation with the cell lysates of LNCaP cell extracts in the presence of NAAG for 2 h at 37°C (1). As shown by the enzyme inhibitory constant (K_i_), the binding affinity was found to increase 5-fold from monovalent compound 1 to bivalent compound 2. There was an 11-fold increase in the affinity for the DOTA-chelated bivalent compound 3 compared to compound 1. Under the same experimental conditions in this study, the K_i_ value of ZJ-43 was reported to be 1.16 nM, indicating the high inhibitory potency of compound 3. ZJ-43 is a urea-based potent inhibitor of NAAG and is used as an internal reference in the assay.

Table 1 PSMA inhibitory activity of compounds 1-3

Compound | Inhibitory constant | 95 percent CI
1 | 0.91 | 0.58–1.45
2 | 0.10 | 0.07–0.16
3 | 0.08 | 0.05–0.12
ZJ-43 | 1.16 | 0.92–1.46

Inhibitory constant: nM

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22207391)]

Biodistribution of [^111^In]3 was determined at 2 h and 24 h after tail vein injection of 74 MBq (20 μCi) [^111^In]3 into nonobese diabetic severe-combined immunodeficient (NOD-SCID) mice that carried both PSMA-positive PC3-PIP and PSMA-negative PC3-flu xenografts (n = 4 mice/group) (1). The percentage of injected dose per gram tissue (% ID/g) was measured ex vivo in selected organs (Table 2). [^111^In]3 displayed PSMA-dependent binding in PC3-PIP xenografts, with continuous accumulation at the tumor site up to 24 h. The PC3-PIP tumor uptake values were 31.93 ± 5.87% ID/g and 34.03 ± 7.53% ID/g at 2 h and 24 h, respectively. The blood, spleen, gastrointestinal tract, kidney, and bladder displayed the highest uptake at 2 h. Steady clearance from the kidneys was observed, from 168.67 ± 14.12% ID/g at 2 h after injection to 66.86 ± 14.22%ID/g at 24 h after injection.

Table 2 Biodistribution data in selected organs in tumor-bearing mice

Organ | 2 h | 24 h
PC3-PIP to PC3-Luc ratio | 203 | 379
Blood | 0.12 ± 0.04 | 0.02 ± 0.01
Liver | 0.19 ± 0.03 | 0.16 ± 0.03
Kidney | 168.67 ± 14.18 | 66.86 ±14.22
Bladder (empty) | 2.61 ± 1.36 | 0.52 ± 0.27
PC3-PIP | 31.93 ± 5.87 | 34.03 ± 7.53
PC3-Luc | 0.16 ± 0.03 | 0.09 ± 0.03

SPECT was performed after tail vein injection of 44.4 MBq (1.2 mCi) [^111^In]3 to one NOD-SCID mouse that carried both PSMA-positive PC3-PIP and PSMA-negative PC3-flu xenografts (1). Radiochemical uptake was followed for up to 192 h after injection. A CT scan was performed before scintigraphy for both anatomical co-registration and attenuation correction. Intense radiotracer uptake was seen only in the PC3-PIP tumors and in the kidneys. Clearance of radioactivity from the kidneys and non-target tissues was more rapid than from the target tumor, such that by 48 h after injection a high tumor/background ratio was observed. The PC3-PIP tumor could still be imaged up to 8 d after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Banerjee S.R., Pullambhatla M., Shallal H., Lisok A., Mease R.C., Pomper M.G. (2011). A modular strategy to prepare multivalent inhibitors of prostate-specific membrane antigen (PSMA). Oncotarget.
2 Conway R.E., Petrovic N., Li Z., Heston W., Wu D., Shapiro L.H. (2006). Prostate-specific membrane antigen regulates angiogenesis by modulating integrin signal transduction. Mol Cell Biol.
3 Foss C.A., Mease R.C., Cho S.Y., Kim H.J., Pomper M.G. (2012). GCPII imaging and cancer. Curr Med Chem.
4 Olson W.C., Heston W.D., Rajasekaran A.K. (2007). Clinical trials of cancer therapies targeting prostate-specific membrane antigen. Rev Recent Clin Trials.
5 Denmeade, S.R., Mhaka, A.M., Rosen, D.M., Brennen, W.N., Dalrymple, S., Dach, I., Olesen, C., Gurel, B., Demarzo, A.M., Wilding, G., Carducci, M.A., Dionne, C.A., Moller, J.V., Nissen, P., Christensen, S.B., and Isaacs, J.T. Engineering a prostate-specific membrane antigen-activated tumor endothelial cell prodrug for cancer therapy. Sci Transl Med. 2012: 4(140): 140ra86.
6 Chen Y., Foss C.A., Byun Y., Nimmagadda S., Pullambhatla M., Fox J.J., Castanares M., Lupold S.E., Babich J.W., Mease R.C., Pomper M.G. (2008). Radiohalogenated prostate-specific membrane antigen (PSMA)-based ureas as imaging agents for prostate cancer. J Med Chem.
7 Chen Y., Pullambhatla M., Foss C.A., Byun Y., Nimmagadda S., Senthamizhchelvan S., Sgouros G., Mease R.C., Pomper M.G. (2011). 2-(3-{1-Carboxy-5-[(6-[18F]fluoro-pyridine-3-carbonyl)-amino]-pentyl}-ureido)-pen tanedioic acid, [18F]DCFPyL, a PSMA-based PET imaging agent for prostate cancer. Clin Cancer Res.
8 Mease R.C., Dusich C.L., Foss C.A., Ravert H.T., Dannals R.F., Seidel J., Prideaux A., Fox J.J., Sgouros G., Kozikowski A.P., Pomper M.G. (2008). N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-4-[18F]fluorobenzyl-L-cysteine, [18F]DCFBC: a new imaging probe for prostate cancer. Clin Cancer Res.